# ^68^Ga-DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_

Chemical name: | ^68^Ga-DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_
Abbreviated name: | ^68^Ga-RM2
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptor (GRPR) with high affinity and specificity (1). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (2). Specific BBN receptors have been identified on CNS and GI tissues, including the pancreas, and on a number of tumor cell lines. The BBN-receptor superfamily includes at least four different subtypes, namely neuromedin B (NMB or BB1), the GRPR subtype (BB2), the BB3 subtype, and the BB4 subtype (3). The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR.

Currently used targeting GRPR peptides are primarily agonists. Therefore, there is a need for GRPR antagonist radioligands. Llinares et al. (4) developed a series of GRPR peptide antagonists. One of them, D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM26), has been found to be a selective GRPR antagonist. A DOTA-Gly-benzoyl group was added to the C-terminus to form DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM1). For evaluation as a single-photon emission computed tomography (SPECT) imaging agent for GRPR, ^111^In has been attached to RM1 to form ^111^In-RM1 (http://www.ncbi.nlm.nih.gov/books/NBK23333/) (5). A new GRPR peptide antagonist, DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM2), has been found to have a higher affinity for GRPR than RM1 and has been labeled with ^68^Ga for positron emission tomography (PET) imaging (6).

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GRPR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925)).
- Articles in OMIM (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=Gastrin-releasing+peptide+receptor+))
- Drug information in FDA (GRPR (http://google-test.fda.gov/search?q=GASTRIN-RELEASING+PEPTIDE+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+synthesis)]

RM2 was prepared by solid-phase peptide synthesis with >70% yield (6). ^68^GaCl_3_ was added to a solution of RM2 (~12 nmol) in aqueous solution (pH 4). The mixture was heated for 2 min at 95°C. The product, ^68^Ga-RM2, had a specific activity of 10 GBq/µmol (0.27 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+in+vitro)]

Mansi et al. (6) performed in vitro inhibition studies of RM1 and RM2 in cultured, GRPR-rich, PC-3 human prostate cells with ^125^I-BBN; Mansi et al. recorded 50% inhibition concentration (IC_50_) values of 35.0 ± 13.0 and 7.7 ± 3.3, respectively. RM2 was able to inhibit the calcium release and receptor internalization induced by BBN.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+rodentia)]

Mansi et al. (6) performed ex vivo biodistribution studies of ~0.2 MBq (5.4 μCi) ^68^Ga-RM2 in nude mice (n = 3/group) bearing PC-3 tumors. Tumor accumulation values for ^68^Ga-RM2 were 9.6 ± 1.5, 14.1 ± 1.9, 14.7 ± 2.1, and 13.6 ± 0.6% injected dose per gram (ID/g) at 20, 60, 80, and 120 min after injection, respectively. ^68^Ga-RM2 exhibited a fast blood clearance, with 0.5% ID/g at 80 min after injection. The tumor/blood ratios were 6, 18, 29, and 43 at 20, 60, 80, and 120 min after injection, respectively. The initial accumulation was high in the pancreas, kidney, pituitary, adrenal, stomach, and intestine at 20 min after injection, with rapid washout by 120 min. The accumulation was low in other tissues. No blocking studies were reported

PET imaging in nude mice bearing LNCaP or PC-3 xenografts was performed with 7 MBq (0.19 mCi) ^68^Ga-RM2 at 60 min after injection. The tumors, kidneys, and urinary bladder were clearly visualized. Preinjection of excess RM2 peptide (20 nmol, 5 min) inhibited the visualization of the tumors at 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga%20RM2+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
3 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
4 Llinares M., Devin C., Chaloin O., Azay J., Noel-Artis A.M., Bernad N., Fehrentz J.A., Martinez J. (1999). Syntheses and biological activities of potent bombesin receptor antagonists. J Pept Res.
5 Mansi R., Wang X., Forrer F., Kneifel S., Tamma M.L., Waser B., Cescato R., Reubi J.C., Maecke H.R. (2009). Evaluation of a 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated bombesin-based radioantagonist for the labeling with single-photon emission computed tomography, positron emission tomography, and therapeutic radionuclides. Clin Cancer Res.
6 Mansi R., Wang X., Forrer F., Waser B., Cescato R., Graham K., Borkowski S., Reubi J.C., Maecke H.R. (2011). Development of a potent DOTA-conjugated bombesin antagonist for targeting GRPr-positive tumours. Eur J Nucl Med Mol Imaging.